# [^18^F]-3-Fluoro-2-(4-((2-nitro-1H-imidazol-1-yl)methyl)-1H-1,2,3-triazol-1-yl)propan-1-ol

Chemical name: | [^18^F]-3-Fluoro-2-(4-((2-nitro-1H-imidazol-1-yl)methyl)-1H-1,2,3-triazol-1-yl)propan-1-ol
Abbreviated name: | [^18^F]-HX4
Synonym:
Agent Category: | Compound
Target: | Hypoxic tissue
Target Category: | Intracellular components
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^18^F
Activation: | Yes
Studies: | - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=2-nitroimidazole&cmd=DetailsSearch)]

The presence of hypoxia is a characteristic feature of solid neoplastic tumors, and it is believed to be related to the aggressive metastasis nature and the development of chemo- and radiotherapy resistance by the tumor (1, 2). In addition, tumor hypoxia is considered to be an important prognostic factor and indicates a poor outcome for the patient (1). Therefore, the hypoxia characterization of tumors is an important diagnostic method for planning cancer treatment(s). Although several invasive and noninvasive methods are available for the detection of hypoxic tumors, these methods have limitations because of the complex blood supply, tumor structure, and oxygen utilization by the tumor cells (3). The invasive method involves placement of oxygen-sensing electrodes in situ and is known to have significant operator variability (1). Among the noninvasive approaches, magnetic resonance imaging with or without contrast agents has been used for the detection of hypoxic tumors, but even this approach does not yield optimal results due to the aberrant blood flow known to exist in different areas of the solid tumors (1). As an alternative, several small molecule tracers or their derivatives (labeled with ^18^F or various copper isotopes) have been developed for use with positron emission tomography (PET) imaging to screen for tumor hypoxia. However, because of their lypophilic nature, these agents produce either low signal/noise ratios due to low uptake by hypoxic lesions and slow clearance from normal tissues (e.g., ^18^F-fluoromisonidazole ([^18^F]FMISO (http://www.ncbi.nlm.nih.gov/bookshelf/br.fcgi?book=micad&part=FMISO)), a 2-nitroimidazole derivative that is frequently used to characterize hypoxic tumors. The mechanisms of activation, biochemistry, and pharmacology of nitroimidazoles are described by Krohn et al. (4)) or do not detect hypoxia in all tumor types (e.g., ^60/61/62/64^Cu-labeled diacetyl-bis(N^4^-methylthiosemicarbazone (http://www.ncbi.nlm.nih.gov/bookshelf/br.fcgi?book=micad&part=Cu-ATSM)) (4).

In an effort to develop a nitroimidazole derivative with superior water solubility and tissue clearance compared to that of [^18^F]-FMISO, a new ^18^F-labeled 2-nitroimidazole derivative, [^18^F]-3-fluoro-2-(4-((2-nitro-1H-imidazol-1-yl)methyl)-1H-1,2,3-triazol-1-yl)propan-1-ol ([^18^F]-HX4), was produced and evaluated for PET imaging of hypoxic tumors in a phase I clinical trial involving six cancer patients (5). Preclinical data for this imaging agent have not been published.

### Other Sources of Information

Clinical trials (http://clinicaltrials.gov/ct2/show/NCT01075399?term=cancer+and+hypoxia&rank=1) with [^18^F]-HX4

Related chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=nitroimidazole+AND+micad%5Bbook%5D&doptcmdl=TOCView&log%24=booksrch&bname=micad)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-HX4%20synthesis&cmd=DetailsSearch)]

The synthesis and labeling of HX4 with ^18^F has been described by van Loon et al. (5). The purification, radiochemical yield, and the time required to synthesize the tracer were not reported. The specific activity of [^18^F]-HX4 was reported to be >14.8 MBq/μmol (>399.9 μCi/μmol), and the final product had a radiochemical purity of >95%. The components of the sterile and pyrogen-free solution used to formulate the imaging agent for human use were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-HX4%20in%20vitro%20studies&cmd=DetailsSearch)]

No publications are currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-HX4%20rodentia&cmd=DetailsSearch)]

No publications are currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-HX4%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-HX4%20Non-Human%20Primates&cmd=DetailsSearch)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

Six individuals (3 females and 3 males, median age 63 years; all had stage IV carcinoma (http://www.cancer.gov/dictionary/?CdrID=45963)) enrolled in a phase I clinical trial and were injected with [^18^F]-HX4 (route of administration not reported). PET images of the largest tumor site were acquired at 30, 60, and 120 min post-injection (p.i.) as described by van Loon et al. (5). The tumor was located on a computed tomographic scan, and the tracer uptake and maximal standardized uptake value (SUV_max_) were determined within the delineated tumor. Subsequently, the tumor/muscle ratios (TMR) were calculated as described (5). In patients who had PET scans with 2-[^18^F]fluoro-2-deoxy-D-glucose ([^18^F]-FDG) before or after the [^18^F]-HX4 image, the tumor uptake of [^18^F]-HX4 was compared to that of [^18^F]-FDG.

The median TMRs were 1.17 (range, 0.20–1.830), 1.25 (range, 0.25–1.67), and 1.40 (range, 0.63–1.98), respectively, at 30, 60, and 120 min p.i. In two patients, the TMR at 120 min p.i. was considerably higher than at 60 min p.i. (data not presented), suggesting that the optimal TMR in these patients would probably be obtained at a time point later than 120 min. In three patients who had [^18^F]-FDG PET scans available, a good correlation was observed between the uptake of [^18^F]-FDG and [^18^F]-HX4.

From this clinical trial, the investigators concluded that, although [^18^F]-HX4 appeared to be suitable for the detection of hypoxic tumors in cancer patients, it was necessary to perform more studies involving patients with an early-stage disease and to acquire images at time points beyond 120 min p.i (5).

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Michalski, M.H. and X. Chen, Molecular imaging in cancer treatment. Eur J Nucl Med Mol Imaging, 2010
2 Torres Martin de Rosales R., Arstad E., Blower P.J. (2009). Nuclear imaging of molecular processes in cancer. Target Oncol.
3 Graves E.E., Maity A., Le Q.T. (2010). The Tumor Microenvironment in Non-Small-Cell Lung Cancer. Semin Radiat Oncol.
4 Krohn K.A., Link J.M., Mason R.P. (2008). Molecular imaging of hypoxia. J Nucl Med.
5 van Loon J., Janssen M.H., Ollers M., Aerts H.J., Dubois L., Hochstenbag M., Dingemans A.M., Lalisang R., Brans B., Windhorst B., van Dongen G.A., Kolb H., Zhang J., De Ruysscher D., Lambin P. (2010). PET imaging of hypoxia using [(18)F]HX4: a phase I trial. Eur J Nucl Med Mol Imaging.